# ^123/131^I-Fab and F(ab')_2_ fragments of anti-integrin α_v_β_5_ monoclonal antibody 14C5

Chemical name: | ^123/131^I-Fab and F(ab')_2_ fragments of anti-integrin α_v_β_5_ monoclonal antibody 14C5
Abbreviated name: | ^123/131^I-Fab/F(ab')_2_-14C5
Synonym:
Agent category: | Antibody Fab fragment
Target: | Integrin α_v_β_5_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^123^I, ^131^I
Activation: | No
Studies: | - In vitro; - Rodents | Structure is currently not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans surrounding connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity. These molecules play a role in inflammation, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM components, which provide a matrix environment for their permeation through the basal lamina and underlying interstitial stroma of the connective tissue. Several ECM adhesion molecules and their protein receptors have been studied extensively for their involvement in tumor invasion and metastasis, including the integrins, lectins, selectins, and cadherins (3).

The monoclonal antibody (mAb) 14C5 recognizes an extracellular membrane antigen expressed on SK-BR-3 human breast tumor cells (4, 5). The mAb 14C5 inhibits the adhesion of tumor cells to ECM and tumor growth. The 14C5 antigen is absent on the cell surface of normal tissues and arteries. However, it is present in high amounts on the cell membrane of invasive breast carcinomas and several other malignant tumors (4). Surprisingly, the 14C5 antigen is markedly expressed on the cell surface of fibroblasts surrounding the tumor cells. The 14C5 antigen is determined to have a molecular weight of ~90 kDa, and 14C5 binds the vascular integrin α_v_β_5_ (6). ^123/131^I-14C5 has been evaluated as a noninvasive agent for radioimmunodetection (7). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (8, 9). Smaller antibody fragments, such as scFv (25 kDa), Fab (50 kDa), or F(ab')_2_ (100 kDa), have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Burvenich et al. (10) compared ex vivo biodistribution and gamma planar imaging of ^123/131^I-Fab-14C5, ^123/131^I-F(ab')_2_-14C5, and ^123/131^I-14C5 in nude mice bearing A549 human lung carcinoma xenografts.

### Related Resource Links:

- Chapters in MICAD (integrin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Integrin+AND+micad%5Bbook%5D), 14C5 (http://www.ncbi.nlm.nih.gov/books/?term=14C5+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_5_ integrin (http://www.ncbi.nlm.nih.gov/gene/3693))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_5_ integrin (http://www.ncbi.nlm.nih.gov/omim/147561))
- Clinical trials (integrin (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (integrin (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20synthesis)]

Fab-14C5, F(ab')_2_-14C5, and 14C5 were labeled with ^123^I, ^125^I, or ^131^I using the Iodogen method as previously described (11). Radiochemical yields were 70%–80% after purification with PD-10 column chromatography (10). Specific activities were ~2.4 GBq/μmol (65 mCi/μmol) with radiochemical purity of >97%. The labeled products were >95% intact after 48 h at 37ºC in buffer.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20in%20vitro)]

Burvenich et al. (11) reported that ^125^I-14C5 bound to SK-BR-3 cells with high affinity, with a dissociation constant (K_d_) value of 0.85 ± 0.17 nM, and SK-BR-3 cells exhibited a high 14C5 antigen expression (B_max_ = 40.6 ± 5.2 pM). In another experiment, the K_d_ values of ^125^I-Fab-14C5 and ^125^I-F(ab')_2_-14C5 were 2.22 ± 0.44 nM and 0.37 ± 0.10 nM, as determined with A549 cells (10), respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20rodentia)]

Burvenich et al. (10) performed blood clearance studies of 13.7 MBq (0.37 mCi) ^131^I-Fab-14C5, ^131^I-F(ab')_2_-14C5, and ^131^I-14C5 in normal mice (n = 3/group) and demonstrated a biexponential clearance from the blood. The biexponential blood clearance of ^131^I-Fab-14C5, ^131^I-F(ab')_2_-14C5, and ^131^I-14C5 was characterized by a fast distribution phase with half-life α (t_1/2,α_) values of 15, 21, and 118 min, respectively, and a slow elimination phase with t_1/2,ß_ values of 439, 627, and 4,067 min, respectively. ^131^I-Fab-14C5 and ^131^I-F(ab')_2_-14C5 exhibited markedly lower t_1/2,α_ and t_1/2,ß_ values than ^131^I-14C5, as Fab and F(ab')_2_ are smaller in size than the whole mAb.

Burvenich et al. (10) performed ex vivo biodistribution studies after injection of 6.9–13.7 MBq (0.185–0.37 mCi) ^131^I-Fab-14C5, ^131^I-F(ab')_2_-14C5, or ^131^I-14C5 in nude mice (n = 3/group) bearing an A549 lung carcinoma at 0.02, 1, 3, 6, 24, and 48 h after tracer injection. The maximum tumor accumulation was observed at 3 h with ^131^I-Fab-14C5 (2.4 ± 0.8% ID/g), at 6 h with ^131^I-F(ab')_2_-14C5 (4.7 ± 0.7% ID/g), and at 24 h with ^131^I-14C5 (10.7 ± 2.2% ID/g). The retention of radioactivity of the whole antibody at 24 h in the liver, kidneys, spleen, heart, lungs, and blood was higher than that of the antibody fragments. On the other hand, the antibody fragments showed an initially high radioactivity (24%–34% ID/g) in the kidneys compared to that of the whole antibody (5.6% ID/g) at 1 h. The maximum tumor/blood ratios for ^131^I-Fab-14C5, ^131^I-F(ab')_2_-14C5, and ^131^I-14C5 were 2.6, 3.5, and 1.3 at 48 h, respectively. Planar gamma images showed that the antibody fragments exhibited improved tumor contrast compared to that of the whole antibody. ^131^I-F(ab')_2_-14C5 and ^131^I-14C5 showed high radioactivity in the liver, whereas ^131^I-Fab-14C5 showed high radioactivity in the kidneys, stomach, and urinary bladder. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=radioisotopes%2014C5%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=14C5%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Coene E., Schelfhout A.M., De Ridder L., De Potter C.R. (1997). Generation of a monoclonal antibody directed against a human cell substrate adhesion molecule and the expression of the antigen in human tissues. Hybridoma.
5 De Potter C.R., Schelfhout A.M., De Smet F.H., Van Damme S., de Ridder L., Dhont E., van Emmelo J. (1994). A monoclonal antibody directed against a human cell membrane antigen prevents cell substrate adhesion and tumor invasion. Am J Pathol.
6 Burvenich I., Schoonooghe S., Vervoort L., Dumolyn C., Coene E., Vanwalleghem L., Van Huysse J., Praet M., Cuvelier C., Mertens N., De Vos F., Slegers G. (2008). Monoclonal antibody 14C5 targets integrin alphavbeta5. Mol Cancer Ther.
7 Lahorte C.M., Bacher K., Burvenich I., Coene E.D., Cuvelier C., De Potter C., Thierens H., Van de Wiele C., Dierckx R.A., Slegers G. (2004). Radiolabeling, biodistribution, and dosimetry of (123)I-mAb 14C5: a new mAb for radioimmunodetection of tumor growth and metastasis in vivo. J Nucl Med.
8 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
9 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
10 Burvenich I.J., Schoonooghe S., Blanckaert P., Bacher K., Vervoort L., Coene E., Mertens N., De Vos F., Slegers G. (2007). Biodistribution and planar gamma camera imaging of (123)I- and (131)I-labeled F(ab')(2) and Fab fragments of monoclonal antibody 14C5 in nude mice bearing an A549 lung tumor. Nucl Med Biol.
11 Burvenich I., Schoonooghe S., Cornelissen B., Blanckaert P., Coene E., Cuvelier C., Mertens N., Slegers G. (2005). In vitro and in vivo targeting properties of iodine-123- or iodine-131-labeled monoclonal antibody 14C5 in a non-small cell lung cancer and colon carcinoma model. Clin Cancer Res.